# ^64^Cu-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-c(RGDyK)-bombesin[7-14]

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-c(RGDyK)-bombesin[7-14]
Abbreviated name: | ^64^Cu-NOTA-RGD-BBN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (14).

Because breast and prostate cancers express both GRPR and α_v_β_3_, Liu et al. (15) designed an RGD-BBN heterodimer in which BBN[7-14] and c(RGDyK) are connected with a glutamate linker (BBN on the Glu side chain γ-carboxylate group and RGD on the Glu side chain α-carboxylate group). A spacer, 11-amino-3,6,9-trioxaundecanoic acid (PEG_3_), was put onto the glutamate α-amino group of Glu-RGD-BBN to increase the hydrophilicity and to relieve the steric hindrance. N-Succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) was used to synthesize [^18^F]SFB-PEG_3_-RGD-BBN for tumor targeting. Liu et al. used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling RGD-BBN to form ^64^Cu-NOTA-RGD-BBN for positron emission tomography (PET) imaging of α_v_β_3_ and GRPR in nude mice bearing human tumors (15, 16).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

RGD-BBN was prepared with solid-phase peptide synthesis with subsequent addition of a NOTA group to form NOTA-RGD-BBN (15). Addition of a NOTA group to RGD-BBN was performed by mixing 2 µmol RGD-BBN with 6 µmol p-SCN-Bz-NOTA in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. NOTA-RGD-BBN was isolated with high-performance liquid chromatography (HPLC) with 52% yield. Measurement with matrix-assisted laser desorption ionization time of flight mass spectrometry indicated the molecular mass to be m/z 2,235.3 (calculated molecular weight, 2,234.6). For ^64^Cu labeling, a solution of 74 MBq (2 mCi) ^64^CuCl_2_ and 5 nmol NOTA-RGD-BBN in acetate buffer (pH 5) was heated for 15 min at 40°C. ^64^Cu-NOTA-RGD-BBN was purified with HPLC with a yield of 92% and a radiochemical purity of >98%. The specific activity was 7.4–14.8 GBq/µmol (0.2–0.4 Ci/µmol). The total preparation time was ~40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Liu et al. (15) performed in vitro inhibition studies of NOTA-RGD-BBN in cultured U87MG cells with ^125^I-c(RGDyK). The 50% inhibition concentration (IC_50_) value was 16.2 ± 2.8 nM. In vitro inhibition studies of NOTA-RGD-BBN were also performed in cultured PC-3 cells with ^125^I-BBN, with an IC_50_ value of 92.8 ± 3.5 nM. The NOTA-RGD-BBN heterodimer exhibited comparable binding affinities for α_v_β_3_ integrin with GRPR and the α_v_β_3_ integrin receptor as the parent RGD and BBN peptides. T47D breast cancer cells were shown to express a moderate level of GRPR and a high level of the α_v_β_3_ integrin. On the other hand, MDA-MB-435 breast cancer cells exhibited a very low level of GRPR and a high level of the α_v_β_3_ integrin. The bindings to both cell lines were specific as the respective cold ligands decreased cell-bound radioactivity to background level. T47D and MDA-MB-435 cells exhibited 5.3% and 2.7% uptake of the incubation dose of ^64^Cu-NOTA-RGD-BBN, respectively, within 120 min of incubation at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Liu et al. (16) performed ex vivo biodistribution studies in normal mice (n = 4/group) at 1 h after injection of 0.37 MBq (0.01 mCi) ^64^Cu-NOTA-RGD-BBN. The organ with the highest accumulation was the pancreas, followed by the liver, kidney, intestine, stomach, blood, and muscle. Co-injection with BBN, c(RGDyK), or BBN+c(RGDyK) experiments were also performed. Little inhibition with c(RGDyK) was observed in most tissues, with the exception of moderate inhibition in the pancreas. BBN exhibited inhibition only in the pancreas, stomach, and intestine. BBN+c(RGDyK) showed inhibition similar to BBN but also showed strong inhibition in the kidney. PET scans were performed after intravenous injection of 3.7 MBq (100 μCi) ^64^Cu-NOTA-RGD-BBN in nude mice (n = 4/group) bearing T47D and MDA-MB-435 human breast tumors at 30, 60, and 120 min (15). The estimated accumulation in the T47D tumors was 3.73 ± 0.81% injected dose per gram (ID/g) at 30 min, and it decreased to 2.33 ± 0.59% ID/g at 1 h and 1.97 ± 0.32% ID/g at 2 h after injection. The estimated accumulation in the MDA-MB-435 tumors was 3.42 ± 1.23% ID/g at 30 min, and it decreased to 1.84 ± 0.44% ID/g at 1 h and 1.47 ± 0.19% ID/g at 2 h after injection. The organs with the highest radioactivity were the kidney (4.32% ID/g at 60 min) and liver (3.28% ID/g at 60 min). The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios were 2, <1, <1, and 3, respectively. On the other hand, [^18^F]FB-PEG_3_-RGD-BBN exhibited higher tumor/organ ratios than ^64^Cu-NOTA-RGD-BBN. In later PET experiments, Liu et al. (16) showed that ^64^Cu-NOTA-RGD-BBN exhibited significantly higher tumor uptake than did ^64^Cu-NOTA-RGD, ^64^Cu-NOTA-BBN, the mixture of ^64^Cu-NOTA-RGD and ^64^Cu-NOTA-BBN, or ^64^Cu-DOTA-RGD-BBN in PC-3 prostate tumors (n = 4/group). The organs with the highest radioactivity were the kidney and liver. However, ^64^Cu-NOTA-RGD-BBN showed lower liver and intestinal activity accumulation than did the BBN tracers. BBN, c(RGDyK), or BBN+c(RGDyK) were co-injected with ^64^Cu-NOTA-RGD-BBN in mice bearing 4T1 breast tumors (n = 3/group). Tumor accumulation at 1 h after injection (2.78% ID/g) was only partially inhibited by either BBN (0.76% ID/g) or c(RGDyK) (1.64% ID/g) alone. However, BBN+c(RGDyK) reduced tumor accumulation to the background level (0.54% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## NIH Support

R01 CA120188, R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
15 Liu Z., Yan Y., Chin F.T., Wang F., Chen X. (2009). Dual integrin and gastrin-releasing peptide receptor targeted tumor imaging using 18F-labeled PEGylated RGD-bombesin heterodimer 18F-FB-PEG3-Glu-RGD-BBN. J Med Chem.
16 Liu Z., Li Z.B., Cao Q., Liu S., Wang F., Chen X. (2009). Small-animal PET of tumors with (64)Cu-labeled RGD-bombesin heterodimer. J Nucl Med.